# ^124^I/^125^I-Fibril-reactive monoclonal antibody

Chemical name: | ^124^I/^125^I-Fibril-reactive monoclonal antibody
Abbreviated name: | ^124^I/^125I^I -11-1F4 MAb
Synonym: | Radioiodinated anti-amyloid fibril monoclonal antibody, ^124^I/^125I^I -c11-1F4 MAb, ^124^I/^125I^I -m11-1F4 MAb
Agent Category: | Antibody
Target: | Amyloid fibril
Target Category: | Antibody to antigen binding
Method of detection: | Positron Emission Tomography (PET) , Single Photon Emission Computed Tomography (SPECT)
Source of signal: | ^124^I, ^125^i
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=625508), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=944925) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=84570) for more information about amyloid fibril

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Fibril-reactive%20monoclonal%20antibody%29%20OR%20%2811-1F4%20monoclonal%20antibody%29%20OR%20%28124I-11-1F4%29)]

^124^I-Fibril-reactive monoclonal antibody (^124^I-11-1F4 MAb) is a radiolabeled antibody that was developed for positron emission tomography (PET) imaging of primary systemic amyloid light –chain (AL) amyloidosis (1). ^124^I is a positron emitter with a physical half-life (t_½_) of 4.2 days. ^125^I-11-1F4 MAb is used for small animal studies. ^125^I-11-1F4 MAb was also used in the animal investigation for small animal single-photon emission computed tomography (SPECT) studies, but ^125^I is a low-energy gamma emitter with a long physical half-life (t_½_) of 60 days.

Amyloidosis describes a heterogeneous group of diseases with a common feature of the extracellular deposition of amyloid proteins in various tissues (2). Amyloid is an amorphous, homogeneous, hyaline-like, eosinophilic substance. Despite its homogeneous appearance, it has a fibrillar structure that consists of linear, non-branching, aggregrated fibrils. The abnormal deposition of this relatively inert fibrillar material in the extracellular compartment of various organs leads to interference with normal functions and destruction of involved tissues and organs. At least 13 different proteins have been identified as human amyloid fibril precursors (2, 3). Primary or idiopathic systemic AL amyloidosis is one of the most common subtypes of amyloidosis. It is a pathologic condition of monoclonal plasma cell dyscrasia (4-6). It is frequently characterized by an abnormal neoplastic proliferation of plasma cells, which synthesize amyloidogenic immunoglobulin light chains. The variable region of the light chain is highly mutated, and this translates into structural heterogeneity and several possible mechanistic pathways of fibril formation (7). The disease may involve the heart, kidney, liver, spleen, tongue, nerves, as well as the vascular system and other body organs/tissues (8)

Monitoring the pathogenesis of these diseases and their responses to treatments is difficult and has traditionally relied on the histologic evaluation of tissue biopsies, and surveys of surrogate physiologic markers. Thus, a specific and noninvasive method for the estimation of amyloid deposition is needed. Hawkins et al. (9-11) demonstrated the possibility of imaging pathologic deposits in vivo with ^123^I-labeled human serum amyloid P component (SAP). Antiproteases are also known to be present in amyloid deposits, and ^99m^Tc-labeled aprotinin (an anti-serine protease) has been studied for AL amyloid imaging with some success in Europe (12, 13).

Solomon et al. (4, 14) developed a murine amyloid-reactive monoclonal antibody, IgG_1к_, 11-1F4 MAb (m11-1F4 MAb), for immunotherapy of AL amyloidosis. This MAb was prepared against a к4 Bence Jones protein. It appeared to react specifically with AL fibrils, regardless of their к or λ constant region isotype or variable region subgroup but did not recognize native (soluble) light chains. The 11-F4 MAb has now been chimerized (c11-1F4 MAb) and is undergoing good manufacturing practice production for phase I and II clinical trials. Wall et al. (1, 15) successfully radioiodinated 11-1F4 MAb with ^124^I and ^125^I for in vivo imaging and provided the basis for future clinical trials of ^124^I-11-1F4 MAb as a potential diagnostic tool in patients with AL amyloidosis and other systemic amyloidoses.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Fibril-reactive%20monoclonal%20antibody%29%20OR%20%2811-1F4%20monoclonal%20antibody%29%20OR%20%28124I-11-1F4%29%20%29AND%20synthesis)]

Murine m11-1F4MAb was produced by the standard hybridoma technique using the SP2/0 hybridoma cell line (16). The antigen was a V_к_ fragment derived from endopeptidase cleavage of a к4 Bence Jones protein.

This murine MAb was chimerized by polymerase chain reaction cloning and sequencing of the heavy and light chain variable region genes. The chimeric c11-1F4 MAb was produced in the CHOdhfr-stable mammalian cell lines that had been transfected with a supervector DNA that encodes the m11-1F4 heavy and light chain variable regions and human heavy and light chain constant regions.

Radioiodination of MAbs with ^125^I or ^124^I was performed by the chloramine-T method (1, 15). Briefly, 0.1−1 mg MAb protein as a concentrated solution was added to 37−74 MBq (1-2 mCi) radioactive iodide in 5 μl of 0.5 M sodium phosphate buffer (pH 7.6). Then 5 μl of freshly prepared chloramine-T (1 mg/ml) was added to the mixture. The reaction was completed within 1 min and was quenched by adding sodium metabisulfite. The iodinated MAb was suspended in phosphate-buffered saline and bovine serum albumin (5 mg/ml) and was purified by size exclusion gel filtration with high-performance liquid chromatography. The radiochemical yield was as high as 80%. Based on the yield, the specific activity was estimated to be 29.6-59.2 MBq/0.1−1 mg (0.8−1.6 mCi/0.1−1 mg). Radiochemical purity of ^125^I/^124^I-Mab was >95−98% using the sodium dodecyl sulfate-polyacrylamide gel electrophoresis. The radioactivity was shown to localize to the heavy and light chains at a ratio of ~ 2:1. The immunoreactivity of the radioiodinated 11-1F4 MAb was 77-79% binding by the 96-well plate radioimmunoassay as well as the bead-conjugated antigen-binding assay.

Wall et al. (15) reported that the succinimidyl-iodobenzoate method produced radioiodinated MAb with 5 to10-fold lower specific activities, and the reaction rate was slower.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Fibril-reactive%20monoclonal%20antibody%29%20OR%20%2811-1F4%20monoclonal%20antibody%29%20OR%20%28124I-11-1F4%29%20%29%20AND%20in%20vitro)]

Wall et al. (1) performed radioimmunoassay by the synthetic Len 1-30 peptide which contained the epitope recognized by 11-1F4 MAb. The Scatchard plot of the data calculated that the dissociation constant (K_d_) of the ^125^I/^124^I-m11-1F4 MAb was ~0.3 nmol/L which was similar to the unlabeled m11-1F4 MAb.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Fibril-reactive%20monoclonal%20antibody%29%20OR%20%2811-1F4%20monoclonal%20antibody%29%20OR%20%28124I-11-1F4%29%20%29%20AND%20rodentia)]

Wall et al. (1) studied the pharmacokinetics and biodistribution of ^125^I-m11-1F MAb in normal mice. Each animal received ~4 MBq/25 μg (0.1 mCi/25 μg) of ^125^I-m11-1F4 MAb by i.v. administration. In the pharmacokinetic study, groups of 6 normal mice were euthanized at 1, 4, 24, 72, and 144 hr after injection. The plasma clearance rate was biexponential with a biological t_½_ of 1.9 ± 1.3 h and 164 ± 67.8 h for the α− and β−components, respectively. At 1 h after injection, ~42% fo the dose remained in the circulation. For ^124^I-m11-1F4 MAb, groups of 3 mice were studied with each mouse receiving an i.v. dose of ~4.5 MBq/10 μg (0.12 mCi/10 μg). The whole-body clearance appeared to fit equivalently to both biexponential and monoexponential curves. Based on the monoexponential curve which produced a more realistic biological t_½_ time, the effective t_½_ times for ^124^I-m11-1F4 MAb and ^125^I-m11-1F4 MAb were determined to be 64 and 158 h, respectively.

Biodistribution studies were performed with ^125^I-m11-1F MAb at 72 h in mice bearing amyloidomas composed of human AL_к_ or AL_λ_ fibrils (1). An i.v. dose of ~11 MBq/10 μg (0.3 mCi/10 μg) was administered to each mouse. In AL_к_ mice, the mean activity levels, measured as the percentage of injected dose per g (% ID/g) in major organs were 22 (amyloidoma), 5.8 (liver), 5 (heart), 4.8 (kidney), 3.9 (spleen), 1.2 (skeletal muscle). The range of radioactivity levels in the AL_к_ amyloidoma was 12−43% ID/g. In contrast, the radioactivity range in the AL_λ_ amyloidoma was 6−12% ID/g with a mean of 9.5% ID/g. No binding was found with the radiolabeled control MOPC-31C antibody to the amyloidoma.

Autoradiography studies were conducted in amyloidoma mice with an i.v. dose of ~11 MBq (0.3 mCi) ^125^I-m11-1F4 MAb. Animals were euthanized at 72 h after injection. Autoradiograms showed that the radiolabeled antibody localized to the amyloid mass. There was more activity in the AL_к_ amyloidomas than in the AL_λ_ amyloidomas. No detectable binding was found with the radiolabeled control antibody.

Small animal single photon emission computed tomography (SPECT)/computed tomography (CT) imaging studies of ^125^I-m11-1F4 MAb were performed in mice bearing 50-mg amyloidomas (1, 15). Each mouse received a dose of ~11.1 MBq/50 μg (0.3 mCi/50 μg) of the radiolabeled antibody and was imaged at 72 h after injection. The images showed that the most intense radioactivity occurred in the amyloidoma that was visualized by the CT scan. There were modest levels of radioactivity in the liver, tongue, and thyroid. When a 60% maximum-intensity threshold for SPECT was used to eliminate the free radioactive iodine background activity, only the AL_к_ and AL_λ_ amyloidomas were visualized. PET/CT imaging studies of ^124^I-m11-1F4 MAb were conducted in a similar manner. Each mouse received an i.v. dose of ~4 MBq/10 μg (0.1 mCi/10 μg) and was imaged at 72 h after injection. The images showed that the radioactivity was primarily confined to the amyloidomas with negligible activity in the blood pool. In both studies, the radiolabeled control antibody showed only minimal activity in the blood pool.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Fibril-reactive%20monoclonal%20antibody%29%20OR%20%2811-1F4%20monoclonal%20antibody%29%20OR%20%28124I-11-1F4%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20shee)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Fibril-reactive%20monoclonal%20antibody%29%20OR%20%2811-1F4%20monoclonal%20antibody%29%20OR%20%28124I-11-1F4%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Fibril-reactive%20monoclonal%20antibody%29%20OR%20%2811-1F4%20monoclonal%20antibody%29%20OR%20%28124I-11-1F4%29%29%20AND%20human)]

No publication is currently available.

## NIH Support

NCI USPHS Research Grant CA-10056, NIBIB RO1 EB000789.

## References

1 Wall J.S., Kennel S.J., Paulus M., Gregor J., Richey T., Avenell J., Yap J., Townsend D., Weiss D.T., Solomon A. (2006). Radioimaging of Light Chain Amyloid with a Fibril-Reactive Monoclonal Antibody. J Nucl Med.
2 Pascali E. (1995). Diagnosis and treatment of primary amyloidosis. Crit Rev Oncol Hematol.
3 Buxbaum J. (1992). Mechanisms of disease: monoclonal immunoglobulin deposition. Amyloidosis, light chain deposition disease, and light and heavy chain deposition disease. Hematol Oncol Clin North Am.
4 Solomon A., Weiss D.T., Wall J.S. (2003). Immunotherapy in systemic primary (AL) amyloidosis using amyloid-reactive monoclonal antibodies. Cancer Biother Radiopharm.
5 Falk R.H., Comenzo R.L., Skinner M. (1997). The systemic amyloidoses. N Engl J Med.
6 Sezer O., Eucker J., Schmid P., Possinger K. (2000). New therapeutic approaches in primary systemic AL amyloidosis. Ann Hematol.
7 Bellotti V., Mangione P., Merlini G. (2000). Review: immunoglobulin light chain amyloidosis--the archetype of structural and pathogenic variability. J Struct Biol.
8 Kyle R.A., Gertz M.A. (1995). Primary systemic amyloidosis: clinical and laboratory features in 474 cases. Semin Hematol.
9 Hawkins P.N., Richardson S., MacSweeney J.E., King A.D., Vigushin D.M., Lavender J.P., Pepys M.B. (1993). Scintigraphic quantification and serial monitoring of human visceral amyloid deposits provide evidence for turnover and regression. Q J Med.
10 Hawkins P.N., Richardson S., Vigushin D.M., David J., Kelsey C.R., Gray R.E., Hall M.A., Woo P., Lavender J.P., Pepys M.B. (1993). Serum amyloid P component scintigraphy and turnover studies for diagnosis and quantitative monitoring of AA amyloidosis in juvenile rheumatoid arthritis. Arthritis Rheum.
11 Hawkins P.N., Wootton R., Pepys M.B. (1990). Metabolic studies of radioiodinated serum amyloid P component in normal subjects and patients with systemic amyloidosis. J Clin Invest.
12 Aprile C., Marinone G., Saponaro R., Bonino C., Merlini G. (1995). Cardiac and pleuropulmonary AL amyloid imaging with technetium-99m labelled aprotinin. Eur J Nucl Med.
13 Schaadt B.K., Hendel H.W., Gimsing P., Jonsson V., Pedersen H., Hesse B. (2003). 99mTc-aprotinin scintigraphy in amyloidosis. J Nucl Med.
14 Solomon A., Weiss D.T., Wall J.S. (2003). Therapeutic potential of chimeric amyloid-reactive monoclonal antibody 11-1F4. Clin Cancer Res.
15 Wall J.S., Paulus M.J., Gleason S., Gregor J., Solomon A., Kennel S.J. (2006). Micro-imaging of amyloid in mice. Methods Enzymol.
16 Hrncic R., Wall J., Wolfenbarger D.A., Murphy C.L., Schell M., Weiss D.T., Solomon A. (2000). Antibody-mediated resolution of light chain-associated amyloid deposits. Am J Pathol.